# Cy5.5-Single-chain Cys-tagged vascular endothelial growth factor-121

Chemical name: | Cy5.5-Single-chain Cys-tagged vascular endothelial growth factor-121
Abbreviated name: | Cy5.5-scVEGF_121_
Synonym:
Agent Category: | Polypeptide
Target: | VEGF receptors
Target Category: | Receptor-ligand binding
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF)]

Optical fluorescence imaging is increasingly used to observe biological functions of specific targets (1, 2) in small animals. However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Vascular endothelial growth factor (VEGF) consists of at least six isoforms with various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (3). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (4). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors on endothelial cells (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4). Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (3).

VEGF receptors were found to be overexpressed in various tumor cells and tumor-associated endothelial cells (5). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (6, 7). Radiolabeled VEGF has been developed as a tracer for imaging solid tumors and angiogenesis in humans (8-10). Cys-tag, a fusion tag comprising 15 amino acids, was developed for site-specific conjugation via the free sulfhydryl group of Cys. Backer et al. (11) prepared a Cys-tagged vector of VEGF_121_ by cloning two single-chain fragments (amino acid sequence 3–112) of VEGF_121_ joining head-to-tail to express as scVEGF, which can be labeled as ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA)-scVEGF (^64^Cu-DOTA-scVEGF), ^99m^Tc-hydrazinonicotinic acid (HYNIC)-scVEGF (^99m^Tc-HYNIC-scVEGF), and Cy5.5-scVEGF for imaging VEGFR expression to study tumor angiogenesis (12). Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^ according to in vitro measurement. Cy5.5-scVEGF is being developed for NIR fluorescence imaging of VEGFR-2 in tumor vasculature.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+synthesis)]

Backer et al. (11) prepared a Cys-tagged vector of VEGF_121_ by cloning two single-chain fragments (amino acid sequence 3–112) of VEGF_121_ joining head-to-tail to express as scVEGF in Escherichia coli. Dithiothreitol-treated scVEGF was incubated with a five-fold molar excess of Cy5.5-maleimide for 90 min (12). Cy5.5-scVEGF was purified with column chromatography. Cy5.5 was identified in the Cys-tag thiol group only and not in the other 16 Cys groups of scVEGF. Hence, there was ~1 Cy5.5/scVEGF. Cy5.5-inVEGF, an inactive control, was prepared by conjugation of 7–8 biotins to Cy5.5-scVEGF.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+and+in+vitro)]

In vitro competition binding studies were performed in 293/KDR cells expressing cloned human VEGFR-2 in competition with the chimeric toxin SLT-VEGF for binding to VEGFR-2 (12). ^64^Cu-DOTA-PEG-scVEGF, DOTA-PEG-scVEGF, HYNIC-scVEGF, and Cy5.5-scVEGF inhibited the binding of SLT-VEGF to VEGFR-2. DOTA-PEG-scVEGF, HYNIC-scVEGF, and Cy5.5-scVEGF stimulated tyrosine phosphorylation of VEGFR-2 in 293/KDR cells in a manner similar to VEGF. Cy5.5-inVEGF exhibited no effects in these two assays. The extensive biotinylation of scVEGF probably destroys the binding capacity of scVEGF. Confocal laser scanning microscopy confirmed intracellular accumulation of Cy5.5-scVEGF in porcine aortic endothelial cells overexpressing VEGFR-2 and not in control cells lacking the receptor.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+rodentia)]

Backer et al. (12) performed in vivo whole-body imaging of mice bearing mouse 4T1 or human MDA-MB-231 mammary adenocarcinoma tumors after i.v. injection of 10 ug of Cy5.5-scVEGF. Persistent fluorescence signal was evident in the tumors for several hours and could be detected up to 7 d after injection. Tumor accumulation of Cy5.5-scVEGF was highly heterogeneous. Co-administration of Cy5.5-scVEGF with 100 ug scVEGF markedly reduced the fluorescence signal. Ex vivo imaging and autoradiography of frozen tumor sections showed that the Cy5.5-scVEGF NIR fluorescence signal intensity in the tumor colocalized with immunoreactivity for VEGFR-1, VEGFR-2, and CD31 (an endothelial cell marker) in endothelial capillary cells. No tumor accumulation of Cy5.5-inVEGF was observed after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+human)]

No publication is currently available.

## NIH Support

R21 EB001946, R43 CA113080, P50 CA114747, CA064436

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
4 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
5 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
6 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
7 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
8 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
9 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
10 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
11 Backer M.V., Patel V., Jehning B.T., Claffey K.P., Backer J.M. (2006). Surface immobilization of active vascular endothelial growth factor via a cysteine-containing tag. Biomaterials.
12 Backer M.V., Levashova Z., Patel V., Jehning B.T., Claffey K., Blankenberg F.G., Backer J.M. (2007). Molecular imaging of VEGF receptors in angiogenic vasculature with single-chain VEGF-based probes. Nat Med.